# 1-[4-(2-[^18^F]Fluoroethoxy)-benzyl]-5-(2-phenoxymethyl-pyrrolidine-1-sulfonyl)-1H-indole-2,3-dione

Chemical name: | 1-[4-(2-[^18^F]Fluoroethoxy)-benzyl]-5-(2-phenoxymethyl-pyrrolidine-1-sulfonyl)-1H-indole-2,3-dione
Abbreviated name: | [^18^F]WC-II-89
Synonym:
Agent category: | Compound
Target: | Caspase-3
Target category: | Enzyme
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=WC-II-89)]

Apoptosis (programmed cell death) plays an important role in the pathophysiology of many diseases, such as cancer, neurodegenerative disorders, vascular disorders, and chronic hepatitis, as well as in the biology of normal cells, such as epithelial cells and immune cells (1). Apoptosis is gene-regulated (2) and is the result of proteolysis of intracellular components by activation of a series of proteolytic enzymes called caspases and changes of plasma membrane structure by translocase, floppase, and scramblase (3-5). As a result, there is rapid redistribution of phosphatidylserine (PS) from the inner membrane leaflet to the outer membrane leaflet, exposing the anionic head group of PS. On the other hand, PS is also accessible for annexin V binding in necrosis because of disruption of the plasma membrane.

Annexin V is a 36-kDa endogenous human protein produced in particular by epithelial cells from many tissues, such as the placenta, umbilical vessels, liver, spleen, kidney, heart, uterus, and skeletal muscle, as well as by erythrocytes, leukocytes, endothelial cells, and platelets (6). Annexin V binds to PS with high affinity (K_d_ = 7 nM) (3, 7, 8). Apoptosis can be induced by chemicals, radiation, cytokines, hormones, and various pathological conditions (5); therefore, the ability to monitor apoptosis in association with disease progression or regression should provide important information for clinical applications. Annexin V has been radiolabeled with ^18^F, ^123^I, ^125^I, and ^99m^Tc for imaging (9-12). However, annexin V is not able to distinguish between apoptosis and necrosis. Caspase ligand may be an attractive alternative for imaging cells undergoing apoptosis because caspases are key enzymes that mediate apoptosis (13). Chu et al. (14) reported that isatin sulfonamide analogs exhibited selective inhibition of caspase-3 and caspase-7 (executioner caspases) over caspase-1, -6, and -8 (initiator caspases). 1-[4-(2-[^18^F]Fluoroethoxy)-benzyl]-5-(2-phenoxymethyl-pyrrolidine-1-sulfonyl)-1H-indole-2,3-dione ([^18^F]WC-II-89), one of the isatin sulfonamide analogs, has been synthesized for imaging caspase-3 activation in apoptosis.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20WC-II-89%20and%20synthesis)]

Zhou et al. (15) report the synthesis of [^18^F]WC-II-89 by nucleophilic displacement of the mesylate group of the mesylate precursor with [^18^F]KF (Kryptofix 2.2.2./K_2_CO_3_). Subsequent high-performance liquid chromatography separation gave a radiochemical yield of >70% with a total synthesis time of <100 min. The specific activity was 55.5 GBq/μmol (1.5 Ci/μmol) at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+WC-II-89+and+in+vitro)]

In vitro caspase enzyme assays using WC-II-89 showed inhibition concentration (IC_50_) values of 9.7 ± 1.3 nM for caspase-3, 23.5 ± 3.5 nM for caspase-7, 3,700 ± 390 nM for caspase-6, >50,000 nM for caspase-1, and >50,000 nM for caspase-8 (15).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20WC-II-89%20and%20rodentia)]

Zhou et al. (15) performed biodistribution studies in normal rats and found high accumulation of radioactivity in the kidney (0.534 ± 0.073% injected dose per gram (ID/g)), followed by the liver (0.378 ± 0.059% ID/g) and lung (0.178 ± 0.032% ID/g) at 60 min after injection of [^18^F]WC-II-89. Pretreatment of rats with cycloheximide (5 mg/kg) to induce apoptosis significantly increased the accumulation of [^18^F]WC-II-89 in the liver (0.733 ± 0.118% ID/g), lung (0.229 ± 0.026% ID/g), spleen (from 0.150 ± 0.048 to 0.427 ± 0.052% ID/g), and muscle (from 0.077 ± 0.008 to 0.104 ± 0.018% ID/g) compared with untreated rats. Western blot studies of apoptotic cells showed increases in the level of cleaved caspase-3 in the liver and spleen of rats that were treated with cycloheximide. The microPET imaging confirmed the approximately two-fold increase in [^18^F]WC-II-89 accumulation in the liver as observed in the biodistribution study. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20WC-II-89%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20WC-II-89%20and%20%28primate%20not%20human%29)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20WC-II-89%20and%20human)]

No publications are currently available.

## NIH Support

HL13851, EB001729, CA121952

## References

1 Thompson C.B. (1995). Apoptosis in the pathogenesis and treatment of disease. Science.
2 Steller H. (1995). Mechanisms and genes of cellular suicide. Science.
3 Thiagarajan P., Tait J.F. (1990). Binding of annexin V/placental anticoagulant protein I to platelets. Evidence for phosphatidylserine exposure in the procoagulant response of activated platelets. J Biol Chem.
4 Song Z., Steller H. (1999). Death by design: mechanism and control of apoptosis. Trends Cell Biol.
5 Blankenberg F.G., Tait J., Ohtsuki K., Strauss H.W. (2000). Apoptosis: the importance of nuclear medicine. Nucl Med Commun.
6 Blankenberg F.G., Strauss H.W. (2001). Will imaging of apoptosis play a role in clinical care? A tale of mice and men. Apoptosis.
7 van Heerde W.L., de Groot P.G., Reutelingsperger C.P. (1995). The complexity of the phospholipid binding protein Annexin V. Thromb Haemost.
8 Tait J.F., Cerqueira M.D., Dewhurst T.A., Fujikawa K., Ritchie J.L., Stratton J.R. (1994). Evaluation of annexin V as a platelet-directed thrombus targeting agent. Thromb Res.
9 Blankenberg F.G. (2004). Recent advances in the imaging of programmed cell death. Curr Pharm Des.
10 Lahorte C., Slegers G., Philippe J., Van de Wiele C., Dierckx R.A. (2001). Synthesis and in vitro evaluation of 123I-labelled human recombinant annexin V. Biomol Eng.
11 Toretsky J., Levenson A., Weinberg I.N., Tait J.F., Uren A., Mease R.C. (2004). Preparation of F-18 labeled annexin V: a potential PET radiopharmaceutical for imaging cell death. Nucl Med Biol.
12 Zijlstra S., Gunawan J., Burchert W. (2003). Synthesis and evaluation of a 18F-labelled recombinant annexin-V derivative, for identification and quantification of apoptotic cells with PET. Appl Radiat Isot.
13 Neuss M., Crow M.T., Chesley A., Lakatta E.G. (2001). Apoptosis in cardiac disease--what is it--how does it occur. Cardiovasc Drugs Ther.
14 Chu W., Zhang J., Zeng C., Rothfuss J., Tu Z., Chu Y., Reichert D.E., Welch M.J., Mach R.H. (2005). N-benzylisatin sulfonamide analogues as potent caspase-3 inhibitors: synthesis, in vitro activity, and molecular modeling studies. J Med Chem.
15 Zhou D., Chu W., Rothfuss J., Zeng C., Xu J., Jones L., Welch M.J., Mach R.H. (2006). Synthesis, radiolabeling, and in vivo evaluation of an 18F-labeled isatin analog for imaging caspase-3 activation in apoptosis. Bioorg Med Chem Lett.